# Multimodal, rhodamine B isothiocyanate-incorporated, silica-coated magnetic nanoparticle–labeled human cord blood–derived mesenchymal stem cells for cell tracking

Chemical name: | Multimodal, rhodamine B isothiocyanate-incorporated, silica-coated magnetic nanoparticle–labeled human cord blood–derived mesenchymal stem cells for cell tracking
Abbreviated name: | MNPs@SiO_2_(RITC)-labeled MSCs
Synonym: | MNPs@SiO_2_(RITC)
Agent Category: | Cells
Target: | Others (cell imaging)
Target Category: | Non-targeted
Method of detection: | Multimodality imaging (MRI and optical imaging)
Source of signal / contrast: | SPIO, RITC
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=mesenchymal+stem+cells+and+cell+tracking+and+imaging)]

Personalized diagnosis and treatment with allogenic or autologous cells are becoming a reality in the field of medicine (1, 2). Cytotoxic or engineered T cells (http://clinicaltrials.gov/ct2/results?term=cytotoxic+T+cells) are under clinical trial for the treatment of hematopoietic or other malignant diseases (1). Contrast agent-tagged macrophages (http://clinicaltrials.gov/ct2/results?term=macrophage+and+imaging) are used as cellular probes to image the early inflammatory processes in macrophage-rich conditions such as inflammation, atherosclerosis, and acute cardiac graft rejection (2). The roles of stem cells (http://clinicaltrials.gov/ct2/results?term=stem+cell) are under intensive investigation in the therapeutic and regenerative medicine such as regenerating cardiomyocytes, neurons, bone, and cartilage (3). Genetically modified cells (http://clinicaltrials.gov/ct2/results?term=genetic+disorders+and+cells) are used to treat genetic disorders (4). With the promising results from these studies, a critical issue is how to monitor the temporal and spatial migration and the homing of these cells, as well as the engraftment efficiency and functional capability of the transplanted cells in vivo (5, 6). Histopathological techniques have only been used to obtain information on the fate of implanted cells at the time of animal euthanization or via biopsy or surgery. To track the real-time changes of cell location, viability, and functional status, cell imaging techniques have been introduced during the last few years. Cells of interest are labeled with reporter genes, fluorescent dyes, or other contrast agents that transform the tagged cells into cellular probes or imaging agents (5-7).

The ability to monitor superparamagnetic iron oxide particles (SPIO) by magnetic resonance imaging (MRI) has been utilized in animal models as well as in a few clinical settings to investigate the fate of labeled cells (5-9). The advantages of using MRI for cell tracking include the high spatial resolution with high anatomic background contrast, the lack of exposure to ionizing radiation, and the ability to follow the cells for months. SPIO particles provide a strong change in signal per unit of metal, in particular on T2- and T2*-weight images. In addition, cell labeling with SPIO nanoparticles is generally nontoxic and does not affect the cell proliferation and differentiation capacity, although a few studies have reported that the stem cells labeled with SPIO lose part of their differentiation capacity in a SPIO concentration–dependent manner (8, 9). An important limitation of MRI is the fact that MRI signals cannot indicate whether cells are dead or alive. It is also unknown whether the MRI signal comes from targeted or labeled cells or from macrophages. Basically, SPIO particles are used to label the target cells by systemic application or by injecting into the tissue area of interest to monitor target cell migration after phagocytosis. SPIO are more frequently used to label the cells in vitro by incorporating into the cells directly. Furthermore, SPIO are usually encapsulated by organic polymers to increase their stability and bio-compatibility, and allow the chemical modification of their surfaces. The fact is that the uptake of different particles varies largely between different cell types (5, 6).

Mesenchymal stem cells (MSCs) represent a heterogeneous subset of pluripotent stromal cells that can be isolated from different adult tissues including adipose tissue, liver, muscle, amniotic fluid, placenta, umbilical cord blood, and dental pulp, although the bone marrow remains the principal source for most preclinical and clinical studies (3, 10, 11). Although MSCs account for only 0.01–0.001% of the total nucleated cells within isolated bone marrow aspirates, they can easily be isolated and expanded in vitro through as many as 40 population doublings in ~8–10 weeks of culture (12). These cells exhibit the potential to differentiate into cells of diverse lineages, such as adipocytes, chondrocytes, osteocytes, myoblasts, cardiomyocytes, neurons, and astrocytes. In addition, MSCs possess remarkable immunosuppressive properties, and they have been shown to be effective against tumor cell growth (13, 14). Yoon et al. generated multimodal, rhodamine B isothiocyanate (RITC)-labeled, silica-coated magnetic nanoparticles (MNPs@SiO_2_(RITC)) and Park et al. labeled the MSCs with the nanoparticles and successfully tracked the labeled cells transplanted into the subcutaneous tissue and liver of the mice (7, 15). Their results indicate that MNPs@SiO_2_(RITC) are biocompatible and useful for human MSC labeling and cell tracking with multimodality imaging.

### Relevant Resource Links

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cell+tracking+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Mesenchymal stem cells under clinical trails (http://clinicaltrials.gov/ct2/results?term=mesenchymal+stem+cells)
- SPIO and cell imaging under clinical trails (http://clinicaltrials.gov/ct2/results?term=SPIO+and+cell+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=multimodal%20+%20RITC%20+%20magnetic%20+mesenchymal)]

Yoon and Park et al. described a three-step synthetic procedure of MNPs@SiO_2_(RITC) nanoparticles in detail (7, 15). The first step was the synthesis of water-soluble, bare cobalt ferrite magnetic nanoparticles with an average size of ~9 nm. This was achieved by co-precipitation of FeCl_3_·6H_2_O and CoCl_2_·6H_2_O in a hot basic NaOH solution. The cobalt ferrite solution was then mixed with polyvinylpyrrolidone solution (PVP) for 24 h at room temperature (20–25°C), and the PVP-stabilized cobalt ferrite nanoparticles were separated with aqueous acetone with centrifugation. As the second step, preparation of the RITC-modified trimethoxysilane was completed with reaction of 3-aminopropyl triethoxysilane and RITC for 17 h in the dark with magnetic stirring and under nitrogen. For the last step, a mixture of tetraethyl orthosilicate and RITC-modified trimethoxysilane was injected into the ethanol solution of PVP-stabilized cobalt ferrite to produce the desired nanoparticles, MNPs@SiO_2_(RITC), with RITC in the silica shell. The thickness of the silica shell was controlled by optimizing the ratio of tetraethyl orthosilicate to magnetic nanoparticles.

The nanoparticles were characterized with various methods (7). The results showed that the average size of the MNPs@SiO_2_(RITC) nanoparticles was ~50 nm with a narrow distribution. The fluorescence decay of RITC encapsulated within silica shell was 14% of the initial intensity, compared with 35% for free RITC after ultraviolet illumination for 24 h, suggesting that RITC embedded within silica was more resistant to photobleaching than free RITC. The fluorescence emission maximum of RITC within silica was shifted to a longer wavelength than that reported for free RITC. MSCs were isolated from human cord blood and expanded in vitro. A concentration of 0.1 mg/ml MNPs@SiO_2_(RITC) in Dulbecco’s modified Eagle medium (low glucose) for 3 h incubation with 60–70% confluence MSCs was determined to be optimal to label the human MSCs (labeling efficiency, 88.98%). No significant change was observed for the light intensity emitted from the labeled cells over a 24-hour period (data not shown). Confocal microscopy showed that the nanoparticles existed in the lysosomes and cytoplasm, and were not present in the nuclei.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=multimodal%20+%20RITC%20+%20magnetic%20+mesenchymal)]

The cytotoxicity of the MNPs@SiO_2_(RITC) was determined after treatment of human MSCs with 0.2–1 mg/ml MNPs@SiO_2_(RITC) for 24, 48, and 72 h (7, 15). More than 90% of the cells were viable for both untreated (control) and treated human MSCs at all examined time points. No floating or swelling cells were observed. The nanoparticle labeling did not induce cell cycle arrest. Neither apoptosis nor necrosis increased in cells treated with MNPs@SiO_2_(RITC) compared with control cells as shown with double staining with annexin V (identifying apoptotic cells) and propidium iodide (revealing nuclear changes). The proliferative rate of labeled MSCs was comparable to that of untreated control groups (all P > 0.05). The surface phenotype of the labeled MSCs was not changed as demonstrated by flow cytometric analysis of the expression of surface antigens, including CD3, CD13, CD20, CD29, CD34, CD38, CD44, CD45, CD56, CD90, CD105, CD117, Lin1, and HLA-ABC. These results strongly indicate that MNPs@SiO_2_(RITC) nanoparticles have no cytotoxic effect on MSCs, at least under culture conditions. Cell passage analysis showed that the RITC signal was still detectable in >90% of the cell population after three passages. After that, the number of cells containing MNPs@SiO_2_(RITC) gradually decreased with each subsequent subculture. However, even after seven passages, ~40% of the cell population still exhibited the RITC signal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=multimodal%20+%20RITC%20+%20magnetic%20+mesenchymal)]

Park et al. first tested the feasibility of detecting the labeled cells with optical imaging and MRI in NOD-SCID mice (7). They injected 1 × 10^6^, 5 × 10^5^, 1 × 10^5^, and 5 × 10^4^ labeled cells into four separate subcutaneous sites of the abdomen (n = 3). Optical imaging clearly showed the presence of human MSCs at the injection sites. MRI showed a strong loss of the signal, presenting dark, distinct areas. As the injected cell numbers decreased, the image distortion decreased.

The investigators then tracked the labeled cells with MRI after injection of 1 × 10^6^ or 1 × 10^5^ human MSCs into the liver via the portal vein. On day 7 after injection, the liver injected with 1 × 10^6^ labeled MSCs showed multiple punctuated dark contrast spots distributed in a very hypointensive area. In the liver injected with 1 × 10^5^ cells, the number and intensity of contrast spots were lower than in the liver with 1 × 10^6^ labeled MSCs, suggesting that the number and intensity of contrast spots were dependent on the injected cell numbers. In the fresh liver tissue sections obtained after animal euthanization on day 7, the fluorescence from nanoparticle-labeled, spindle-shaped human MSCs was clearly visible, and the fluorescence signal in the paraffin-embedded tissue sections persisted for >6 months under general storage conditions (data not shown).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Cesco-Gaspere M., Morris E., Stauss H.J. (2009). Immunomodulation in the treatment of haematological malignancies. Clin Exp Med.
2 Eisenblatter M., Ehrchen J., Varga G., Sunderkotter C., Heindel W., Roth J., Bremer C., Wall A. (2009). In vivo optical imaging of cellular inflammatory response in granuloma formation using fluorescence-labeled macrophages. J Nucl Med.
3 Mathiasen A.B., Haack-Sorensen M., Kastrup J. (2009). Mesenchymal stromal cells for cardiovascular repair: current status and future challenges. Future Cardiol.
4 Bachoud-Levi A.C. (2009). Neural grafts in Huntington's disease: viability after 10 years. Lancet Neurol.
5 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
6 Hoehn M., Wiedermann D., Justicia C., Ramos-Cabrer P., Kruttwig K., Farr T., Himmelreich U. (2007). Cell tracking using magnetic resonance imaging. J Physiol.
7 Park, K.S., J. Tae, B. Choi, Y.S. Kim, C. Moon, S.H. Kim, H.S. Lee, J. Kim, J.S. Kim, J. Park, J.H. Lee, J.E. Lee, J.W. Joh, and S. Kim, Characterization, in vitro cytotoxicity assessment, and in vivo visualization of multimodal, RITC-labeled, silica-coated magnetic nanoparticles for labeling human cord blood-derived mesenchymal stem cells. Nanomedicine, 2009
8 Arbab A.S., Bashaw L.A., Miller B.R., Jordan E.K., Lewis B.K., Kalish H., Frank J.A. (2003). Characterization of biophysical and metabolic properties of cells labeled with superparamagnetic iron oxide nanoparticles and transfection agent for cellular MR imaging. Radiology.
9 Arbab A.S., Liu W., Frank J.A. (2006). Cellular magnetic resonance imaging: current status and future prospects. Expert Rev Med Devices.
10 Ehrchen J., Helming L., Varga G., Pasche B., Loser K., Gunzer M., Sunderkotter C., Sorg C., Roth J., Lengeling A. (2007). Vitamin D receptor signaling contributes to susceptibility to infection with Leishmania major. FASEB J.
11 Sadan O., Melamed E., Offen D. (2009). Bone-marrow-derived mesenchymal stem cell therapy for neurodegenerative diseases. Expert Opin Biol Ther.
12 Huang D.M., Hsiao J.K., Chen Y.C., Chien L.Y., Yao M., Chen Y.K., Ko B.S., Hsu S.C., Tai L.A., Cheng H.Y., Wang S.W., Yang C.S. (2009). The promotion of human mesenchymal stem cell proliferation by superparamagnetic iron oxide nanoparticles. Biomaterials.
13 Loebinger M.R., Kyrtatos P.G., Turmaine M., Price A.N., Pankhurst Q., Lythgoe M.F., Janes S.M. (2009). Magnetic resonance imaging of mesenchymal stem cells homing to pulmonary metastases using biocompatible magnetic nanoparticles. Cancer Res.
14 Kuhn N.Z., Tuan R.S. (2010). Regulation of stemness and stem cell niche of mesenchymal stem cells: implications in tumorigenesis and metastasis. J Cell Physiol.
15 Yoon T.J., Kim J.S., Kim B.G., Yu K.N., Cho M.H., Lee J.K. (2005). Multifunctional nanoparticles possessing a "magnetic motor effect" for drug or gene delivery. Angew Chem Int Ed Engl.